# 2-(2-Nitro-1H-imidazol-1-yl)-N-(2,2,3,3,3-[^18^F]pentafluoropropyl)-acetamide

Chemical name: | 2-(2-nitro-1H-imidazol-1-yl)-N-(2,2,3,3,3-[^18^F]pentafluoropropyl)-acetamide
Abbreviated name: | [^18^F]EF5
Synonym: | [^18^F]-2-(2-nitro-1H-imidazol-1-yl)-N-(2,2,3,3,3-[^18^F]pentafluoropropyl)-acetamide
Agent Category: | Compound
Target: | Hypoxic cells
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20EF5%5BAll%20Fields%5D)]

Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy, and its accurate diagnosis is considered a very important and urgent problem to address. This has led to the search for and development of hypoxia-targeted imaging techniques and non-invasive markers of tumor hypoxia. Among those, ^18^F-labeled nitroimidazoles - used in conjunction with positron emission tomography (PET) – offer a alternative that is less invasive and less prone to sampling errors than the Eppendorf (oxygen) electrode method (1, 2).

Fluoromisonidazole ([underlined: []^[underlined: 18]^[underlined: F]FMISO]) is the nitroimidazole derivative most widely used with PET. Novel 2-nitroimidazoles, such as ^18^F-labeled fluoroetanidazole ([underlined: []^[underlined: 18]^[underlined: F]FETA]) (3), fluoroerythronitroimidazole ([underlined: []^[underlined: 18]^[underlined: F]FETNIM]) (4), 4-bromo-1-(3-fluoropropyl)-2-nitroimidazole ([underlined: 4-Br[]^[underlined: 18]^[underlined: F]FPN]) (5), and 2-(2-nitroimidazol-1H-yl)-N-(3-fluoropropyl)acetamide ([underlined: []^[underlined: 18]^[underlined: F]EF1]) (6), are currently under investigation as PET markers for hypoxia.

The pentafluorinated molecule EF5 (2-(2-nitro-1H-imidazol-1-yl)-N-(2,2,3,3,3-pentafluoropropyl)-acetamide), previously used for measurement of hypoxia by immunohistochemistry (7) and flow cytometry (8), is currently being investigated as a PET agent for hypoxia. [^18^F]EF5 has the advantage of being more lipophilic than [^18^F]EF1 (octanol-water partition coefficient of 5.7 for [^18^F]EF5 versus 0.35 for [^18^F]EF1) because of its multiple fluorine atoms. [^18^F]EF5 can easily access all tissues, including those in the nervous system.

The oxygen-dependent metabolism of [^18^F]EF5 is an intracellular process consisting of a series of one-electron reductions. The nitro-radical anion produced in the first reduction step is very reactive toward oxygen, leaving no substrate for the second step of the reduction process. In contrast, a low-oxygen environment induces further reductive reactions that ultimately lead either to the formation of reactive products that can covalently bind to cell components or to charged species that diffuse slowly out of the tissues (1). The reactive products observed during this multistep process include nitroso (2e^-^), hydroxylamine (4e^-^), and amine (6e^-^) derivatives. When fragmentation of the imidazole ring occurs, reactive portions of the molecule, such as glyoxal, bind to macromolecular components of cells in tissues and tumors (2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20EF5%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^18^F]EF5 can be produced by direct fluorination of the precursor 2-(2-nitro-1H-imidazol-1-yl)-N-(2,3,3-trifluoroallyl)-acetamide by [^18^F]F_2_ in trifluoroacetic acid, as described by Dolbier et al. (9). The yield obtained by this method is greater than 10%.

Synthesis details have also been reported by Ziemer et al. (10). Their described procedure also involves adding fluorine gas across the double bond of an allyl precursor in trifluoroacetic acid at 0 °C. After evaporation under vacuum, the products are purified by high-performance liquid chromatography (HPLC). After dissolution in physiologic saline, the purified radioactive drug is added to unlabeled EF5. The maximum specific activity for [^18^F]EF5 synthesis is about 37 × 10^3^ MBq (1,000 mCi)/mmol (when using 7400 MBq (200 mCi) of radioactivity in 70 µmol of fluorine carrier, and assuming a 30% labeling efficiency).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF5%20AND%20PET%20AND%20in%20vitro)]

No in vitro study using the PET agent [^18^F]EF5 has been reported in the literature to date. Nevertheless, data on the distribution and levels of EF5 binding using fluorescence immunohistochemical techniques have been reported for human head-and-neck and cervical squamous cancer cells (11). In those studies, the maximum rate of in situ binding varied by a factor of 6.7 between the lowest (24.8) and the highest (160.3) on an absolute fluorescence scale. Intratumoral heterogeneity was observed for tumors with high binding regions. In contrast, this heterogeneity was minimal for tumors with minimal binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF5%20AND%20rodentia%5BMeSH%5D)]

Biodistribution studies using male Fischer rats bearing Morris 7777 (Q7) tumors and 9L glioma were performed by Ziemer et al. (10). The rats were injected with approximately 50-100 μCi of [^18^F]EF5 and 100 μmol/kg of nonradioactive EF5 (used as added carrier). Images were taken at 10, 60, 120, and 180 min post injection through the femoral vein. [^18^F]EF5 was shown to be distributed fairly uniformly, with activity uptake increasing over time in the kidneys and gastrointestinal (GI) tract. This increase suggests that [^18^F]EF5 is excreted via the urinary system, consistent with prior research studies of EF5 in rodents (12). In contrast, the activity in the liver appeared to be roughly constant and decreasing slowly over time.

At 60 min post injection, the values for the ratio of activity in organs to activity in muscle were as follows: 2.0 (liver), 2.5 (kidney), and 2.7 (GI tract). At 120 min post injection, those ratios were 1.9 (liver), 2.8 (kidney), and 3.9 (GI tract) (as reported in figure 2 of Ziemer et al. (10)). For Q7 tumor -bearing rats, the following tumor/muscle activity ratios (TMR) were obtained: 1.5 (kidney), 1.4 (liver), and 1.3 (GI tract) at 60 min post injection; and 1.2 (kidney), 1.7 (liver), and 1.6 (GI tract) at 120 min post injection (as reported in figure 3 of Ziemer et al. (10)).

Additional measurements of TMR values based on gamma counts led to consistently higher values than those obtained with PET imaging. As an example, the TMR value obtained for a Q7 tumor of size 14 × 14 × 14 = 2,744 mm^3^ was 1.73 with PET imaging but 2.43 when gamma-counted. This difference was thought to be likely due to the small tumor size and the partial volume effect.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF5%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF5%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF5%20AND%20human)]

No publication reporting on [^18^F]EF5 as a PET agent in human studies is currently available. Nevertheless, EF5 is approved for use in humans and is currently in phase II clinical trials using antibody techniques for the detection of hypoxic cells (13).

## References

1 Nunn A, Linder K, Strauss HW. (1995). Nitroimidazoles and imaging hypoxia. Eur J Nucl Med.
2 Hodgkiss RJ. (1998). Use of 2-nitroimidazoles as bioreductive markers for tumour hypoxia. Anticancer Drug Des.
3 Rasey JS, Hofstrand PD, Chin LK, Tewson TJ. (1999). Characterization of [18F]fluoroetanidazole, a new radiopharmaceutical for detecting tumor hypoxia. J Nucl Med.
4 Yang DJ, Wallace S, Cherif A, Li C, Gretzer MB, Kim EE, Podoloff DA. (1995). Development of F-18-labeled fluoroerythronitroimidazole as a PET agent for imaging tumor hypoxia. Radiology.
5 Yamamoto F, Aoki M, Furusawa Y, Ando K, Kuwabara Y, Masuda K, Sasaki S, Maeda M. (2002). Synthesis and evaluation of 4-bromo-1-(3-[18F]fluoropropyl)-2-nitroimidazole with a low energy LUMO orbital designed as brain hypoxia-targeting imaging agent. Biol Pharm Bull.
6 Kachur AV, Dolbier WR, Evans SM, Shiue CY, Shiue GG, Skov KA, Baird IR, James BR, Li AR, Roche A, Koch CJ. (1999). Synthesis of new hypoxia markers EF1 and [18F]-EF1. Appl Radiat Isot.
7 Evans SM, Joiner B, Jenkins WT, Laughlin KM, Lord EM, Koch CJ. (1995). Identification of hypoxia in cells and tissues of epigastric 9L rat glioma using EF5. Br J Cancer.
8 Evans SM, Jenkins WT, Joiner B, Lord EM, Koch CJ. (1996). 2-Nitroimidazole (EF5) binding predicts radiation resistance in individual 9L s.c. tumors. Cancer Res.
9 Dolbier WR, Li AR, Koch CJ, Shiue CY, Kachur AV. (2001). [18F]-EF5, a marker for PET detection of hypoxia: synthesis of precursor and a new fluorination procedure. Appl Radiat Isot.
10 Ziemer LS, Evans SM, Kachur AV, Shuman AL, Cardi CA, Jenkins WT, Karp JS, Alavi A, Dolbier WR, Koch CJ. (2003). Noninvasive imaging of tumor hypoxia in rats using the 2-nitroimidazole 18F-EF5. Eur J Nucl Med Mol Imaging.
11 Evans SM, Hahn S, Pook DR, Jenkins WT, Chalian AA, Zhang P, Stevens C, Weber R, Weinstein G, Benjamin I, Mirza N, Morgan M, Rubin S, McKenna WG, Lord EM, Koch CJ. (2000). Detection of hypoxia in human squamous cell carcinoma by EF5 binding. Cancer Res.
12 Laughlin KM, Evans SM, Jenkins WT, Tracy M, Chan CY, Lord EM, Koch CJ. (1996). Biodistribution of the nitroimidazole EF5 (2-[2-nitro-1H-imidazol-1-yl]-N-(2,2,3,3,3-pentafluoropropyl) acetamide) in mice bearing subcutaneous EMT6 tumors. J Pharmacol Exp Ther.
13 Koch CJ, Hahn SM, Rockwell K, Covey JM, McKenna WG, Evans SM. (2001). Pharmacokinetics of EF5 [2-(2-nitro-1-H-imidazol-1-yl)-N-(2,2,3,3,3-pentafluoropropyl) acetamide] in human patients: implications for hypoxia measurements in vivo by 2-nitroimidazoles. Cancer Chemother Pharmacol.